# 4-(3-Cyclopentoxy-4-[^11^C]methoxy-phenyl)pyrrolidin-2-one

Chemical name: | 4-(3-Cyclopentoxy-4-[^11^C]methoxy-phenyl)pyrrolidin-2-one
Abbreviated name:
Synonym: | [^11^C]Rolipram
Agent Category: | Compound
Target: | Phosphodiesterase type IV
Target Category: | Enzyme binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20rolipram)]

Phosphodiesterases (PDEs) are composed of at least 11 families of enzymes that hydrolyze cyclic 3´,5´-adenosine monophosphate (cAMP) and/or 3´,5´-guanosine monophosphate (cGMP) to the corresponding inactive 5´-AMP and 5´-GMP, respectively (1, 2). These second-messenger cyclic nucleotides are formed in response to stimuli (such as hormones, neurotransmitters, and cytokines) to regulate cellular functions. PDEs are essential in the termination of cellular responses via their degradation of cyclic nucleotides. PDE type-4 (PDE4) is Ca^2+^/calmodulin independent, cAMP specific, and found mainly in the kidney, brain, liver, lung, Sertoli cells, and lymphoid cells (2, 3). There are four subtypes of PDE4 enzymes. PDE4 activity and density are up-regulated by increasing cAMP levels through phosphorylation with protein kinase A (4). PDE4 inhibitors have been studied in the treatment of neuropsychiatric disorders (depression and dementia of Alzheimer’s disease) (5-7) and inflammatory diseases (asthma) (8, 9).

R/S-4-(3-Cyclopentoxy-4-methoxy-phenyl)pyrrolidin-2-one (R/S-rolipram) was found to be a specific inhibitor of all four subtypes of PDE4 with high affinity (K_d_ = 1-2 nM) (10). DaSilva et al. (11) reported IC_50_ values for R-, R/S-, and S-rolipram of 2-5, 5-7, and 42-95 nM, respectively. PDE4 is highly expressed in rat brain (B_max_ >100 fmol/mg of tissue) (10, 12). The clinical program for rolipram was ultimately suspended in humans using pharmacologic doses because of its side effects, such as emesis and sedation (13). However, the action of the compound on PDE4 would be useful as a tool to better understand the biochemical basis of depression and the role that PDE4 inhibitors may play in antidepressant therapy (14). At least one study using positron emission tomography (PET) to study R-[^11^C]rolipram in humans was reported in 2002. R-[^11^C]Rolipram is being developed as a PET agent for the non-invasive study of PDE4 in the brain in small animals.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20synthesis)]

Lourenco et al. (15) synthesized R/S-[^11^C]rolipram as a mixture of R and S enantiomers by alkylation of the desmethyl precursor with [^11^C]methyl iodide. Subsequent separation by high-performance liquid chromatography gave a radiochemical purity >95%. The specific activity was >14.8 GBq/μmol (>400 Ci/mmol) at time of injection. No yield was reported (15). Later, DaSilva et al. (11) described the syntheses of S-[^11^C]rolipram from S-desmethyl-rolipram and R-[^11^C]rolipram from R-desmethyl-rolipram with [^11^C]methyl iodide. The ^11^C enantiomers were prepared with a radiochemical yield of 45-75% (decay-corrected) based on [^11^C]methyl iodide. Total synthesis time was 30 min. Radiochemical purity was >99% with specific activities of 18.5-92.5 GBq/μmol (0.5-2.5 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20in%20vitro)]

R/S-[^3^H]Rolipram binds with high affinity (K_d_ = 2.52 ± 0.47 nM) to sections of rat brain in vitro (10). Association of R/S-[^3^H]rolipram to brain sections is rapid (47% of specific binding in the first minute). Dissociation of R/S-[^3^H]rolipram exhibits non-first-order kinetics (three-component model; t_1/2_ = 2.5 min, 50 min, and 6 h, respectively). R/S-[^3^H]Rolipram binding to the brain sections was reduced by several PDE inhibitors to the level of nonspecific binding (IC_50_ = 0.9 nM for R-rolipram, 1.5 nM for R/S-rolipram, 11 nM for Ro 20-1724, and 35 nM for ICI 63.197), but not by medazepam (IC_50_ = 240 nM), diazepam (IC_50_ = 1200 nM), and IBMX (IC_50_ = 3800 nM). In vitro autoradiography revealed high binding site densities (in decreasing binding order) in the olfactory bulb, lateral septal nucleus, frontal cortex, subiculum, cerebellum, and hippocampus. Most of the labeled structures are part of the limbic system. Schneider et al. (16) reported previously that membrane-bound PDE4 and soluble PDE4 enzymes in rat brain homogenates exhibited K_d_ values of 1.2 and 2.4 nM, respectively, and B_max_ values of 19.3 and 23.6 pmol/g tissue. The R-enantiomer of rolipram was 20 times more effective than the S-enantiomer in displacing R/S-[^3^H]rolipram from the brain membranes. The authors found that the B_max_ for human cerebellar cortex membranes was ~50% that for the frontal cortex membranes. Parker et al. (17) reported a calculated affinity ratio of 8 for rat cortical membranes in R-[^3^H]rolipram and S-[^3^H]rolipram competition assays.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20rodentia)]

Biodistribution studies in normal rats showed high accumulation of radioactivity in the liver, followed by the brain, lung, and heart at 5 min after injection of R/S-[^11^C]rolipram (15). Radioactivity from the tracer was low in the blood. R/S-[^11^C]Rolipram accumulation was higher in the frontal cortex (0.57 ± 0.12% injected dose (ID)/g) and lower in the brain stem (0.26 ± 0.06% ID/g) at 45 min post injection, as predicted by the density of PDE4 enzymes. Coadministration of unlabeled R/S-rolipram decreased the accumulation of radioactivity in the brain regions, suggesting specific binding. Pretreatment with high doses of vinpocetine (a PDE1 inhibitor) or desipramine (a noradrenalin reuptake inhibitor) did not inhibit R/S-[^11^C]rolipram accumulation in the brain regions, suggesting selectivity for PDE4 enzymes.

Fujita et al. (18) reported PET studies of the accumulation of enantiomeric [^11^C]rolipram in the brains of normal rats, using a two-compartment model with an arterial input function for analyses. No significant differences in metabolism of the ^11^C enantiomers were observed in blood. Both ^11^C enantiomers remained 97% intact in the brain; however, the R-enantiomer was retained to a significantly greater extent than the S-enantiomer, and its distribution in the brain was less uniform than that of the S-enantiomer. Coadministration of unlabeled R-rolipram decreased the accumulation of R-[^11^C]rolipram radioactivity in various brain regions to that of S-[^11^C]rolipram. The average total distribution volume of all brain regions for S-[^11^C]rolipram was only 14% that of R-[^11^C]rolipram. The observed differences are consistent with the reported greater in vitro affinity of the R-enantiomer for PDE4 binding sites compared with the S-enantiomer.

The selective PDE4 inhibitor (R)-rolipram labeled with C-11 was tested in vivo in rats to analyze changes in PDE4 levels following drug treatments that increase synaptic noradrenaline (NA), serotonin (5HT), histamine (HA) and dopamine (DA) levels. We hypothesized that increasing synaptic neurotransmitter levels and subsequent cAMP-mediated signaling would significantly enhance (R)-[^11^C]rolipram retention and specific binding to PDE4 in vivo. Pre-treatments were performed 3 h prior to tracer injection, and rats were sacrificed 45 min later. Biodistribution studies revealed a dose-dependent increase in (R)-[^11^C]rolipram uptake following administration of the monoamine oxidase (MAO) inhibitor tranylcypromine, NA and 5HT reuptake inhibitors (desipramine [DMI], maprotiline; and fluoxetine, sertraline, respectively), and the HA H_3_ receptor antagonist (thioperamide), but not with DA transporter blockers GBR 12909, cocaine or DA D_1_ agonist SKF81297. Significant increases in rat brain and heart reflect changes in PDE4 specific binding (total − non-specific binding [coinjection with saturating dose of (R)-rolipram]). These results demonstrate that acute treatments elevating synaptic NA, 5HT and HA, but not DA levels, significantly enhance (R)-[^11^C]rolipram binding. Use of (R)-[^11^C]rolipram and positron emission tomography as an index of PDE4 activity could provide insight into understanding disease states with altered NA, 5HT and HA concentrations.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Parker et al. (17) obtained PET images of the brain in pigs after injection of R-[^11^C]rolipram or S-[^11^C]rolipram with coadministration of either unlabeled R- or S-rolipram. In all studies, R-[^11^C]rolipram exhibited a higher affinity for the PDE4 enzymes in various brain regions compared with S-[^11^C]rolipram. The calculated affinity ratios from distribution volumes were 12.5 and 14.7 for R- and S-[^11^C]rolipram, respectively. The occipital cortex exhibited the highest distribution volume, followed by the frontal cortex, thalamus, and cerebellum.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20%28primate%20not%20human%29)]

Using PET, Parker et al. (19) obtained serial brain scans in conscious monkeys after injection of R- or S-[^11^C]rolipram with 0, 0.1, 0.3, and 1 mg/kg methamphetamine (a dopamine release inducer) pretreatment. Accumulation of radioactivity in the striata was enhanced in a dose-dependent manner corresponding to dopamine levels in striatal extracellular fluid measured with microdialysis. Administration of scopolamine,a N-methyl-D-aspartic acid (NMDA) receptor inhibitor), also enhanced PDE4 activity without any apparent changes in the dopamine levels. Scopolamine was reported to enhance dopamine release and reuptake simultaneously (20). The enhancements of PDE4 activity by methamphetamine and scopolamine at 1 mg/kg were abolished by preadministration of the D_1_ antagonist (R)-(+)-8-chloro-2,3,4,5-tetrahydro-3-methyl-5-phenyl-1H-3-benzazepin-7-ol (SCH23390; 2 mg/kg) but not by the D_2_ antagonist raclopride. Both methamphetamine and scopolamine had no effects on [^11^C]SCH23390 striatal binding. These data suggest that dopamine in the synaptic cleft may activate D_1_ receptor-coupled PDE4 activity.

Harada et al. (21) used PET to study the age-related changes in striatal dopamine D_1_ receptor binding and its related PDE4 activity in the living brains of conscious young (6.4 ± 1.8 years of age) and older (19.5 ± 3.3 years of age) monkeys. [^11^C]SCH23390 was used for quantitative analysis of D_1_ receptors, and PDE4 activity, as an index of the cAMP system, was estimated by two scans with R- and S-[^11^C]rolipram. Significant age-related decreases in D_1_ receptor binding were observed in the striatum and frontal cortex. Analysis of the uptake of R- and S-[^11^C]rolipram indicated age-related decreases in PDE4 activity, with decreases of 22.0 and 25.2% in the striatum and frontal cortex, respectively, whereas there were no significant changes in the cerebellum, which had lower accumulation than the striatum and frontal cortex. Pretreatment with the dopamine D_1_ receptor antagonist SCH23390 (0.2, 0.6, and 2 mg/kg) suppressed the PDE4 activities in the striatum and frontal cortex in both age groups in a dose-dependent manner. However, suppression by SCH23390 was more pronounced in young than in older monkeys (P <0.05). These results demonstrate that the striatal PDE4 activity as well as its functional response to dopamine D_1_ antagonist showed age-related impairment in the brain.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Rolipram%20and%20human)]

DaSilva et al. (11) reported on PET studies in 11 healthy volunteers after injection of 370 MBq (10 mCi) of R-[^11^C]rolipram. Regional brain accumulation was rapid initially and peaked at ~10 min, followed by a gradual decrease. High levels of R-[^11^C]rolipram radioactivity were observed in the thalamus, which then decreased to levels similar to the binding in the cortical and striatal areas at 40 min. The peak accumulation in the thalamus corresponded to ~5% ID/L. Lower accumulation was observed in the striatum (4.5% ID/L), prefrontal cortex (4.0% ID/L), and cerebellum (3.5% ID/L). Kinetic analysis revealed that a two-tissue compartment model with arterial function input can be used to assess the brain accumulation of R-[^11^C]rolipram.

Internal dosimetry data for R-[^11^C]rolipram in humans are not available in the literature.

## Supplemental Information

[Disclaimers]

Chemistry

Synthesis Protocol

Animal Dosimetry

## NIH Support

Intramural Research Program

## References

1 Sutherland E.W., Rall T.W. (1958). Fractionation and characterization of a cyclic adenine ribonucleotide formed by tissue particles. J Biol Chem.
2 Essayan D.M. (2001). Cyclic nucleotide phosphodiesterases. J Allergy Clin Immunol.
3 Houslay M.D. (2001). PDE4 cAMP-specific phosphodiesterases. Prog Nucleic Acid Res Mol Biol.
4 Conti M., Nemoz G., Sette C., Vicini E. (1995). Recent progress in understanding the hormonal regulation of phosphodiesterases. Endocr Rev.
5 Duman R.S., Nakagawa S., Malberg J. (2001). Regulation of adult neurogenesis by antidepressant treatment. Neuropsychopharmacology.
6 Fleischhacker W.W., Hinterhuber H., Bauer H., Pflug B., Berner P., Simhandl C., Wolf R., Gerlach W., Jaklitsch H., Sastre-y-Hernandez M., et al. (1992). A multicenter double-blind study of three different doses of the new cAMP-phosphodiesterase inhibitor rolipram in patients with major depressive disorder. Neuropsychobiology.
7 Gong B., Vitolo O.V., Trinchese F., Liu S., Shelanski M., Arancio O. (2004). Persistent improvement in synaptic and cognitive functions in an Alzheimer mouse model after rolipram treatment. J Clin Invest.
8 Dyke H.J., Montana J.G. (2002). Update on the therapeutic potential of PDE4 inhibitors. Expert Opin Investig Drugs.
9 Kim E., Chun H.O., Jung S.H., Kim J.H., Lee J.M., Suh B.C., Xiang M.X., Rhee C.K. (2003). Improvement of therapeutic index of phosphodiesterase type IV inhibitors as anti-Asthmatics. Bioorg Med Chem Lett.
10 Kaulen P., Bruning G., Schneider H.H., Sarter M., Baumgarten H.G. (1989). Autoradiographic mapping of a selective cyclic adenosine monophosphate phosphodiesterase in rat brain with the antidepressant [3H]rolipram. Brain Res.
11 DaSilva J.N., Lourenco C.M., Meyer J.H., Hussey D., Potter W.Z., Houle S. (2002). Imaging cAMP-specific phosphodiesterase-4 in human brain with R-[11C]rolipram and positron emission tomography. Eur J Nucl Med Mol Imaging.
12 Borisy F.F., Hwang P.N., Ronnett G.V., Snyder S.H. (1993). High-affinity cAMP phosphodiesterase and adenosine localized in sensory organs. Brain Res.
13 Heaslip R.J., Evans D.Y. (1995). Emetic, central nervous system, and pulmonary activities of rolipram in the dog. Eur J Pharmacol.
14 O'Donnell J.M., Zhang H.T. (2004). Antidepressant effects of inhibitors of cAMP phosphodiesterase (PDE4). Trends Pharmacol Sci.
15 Lourenco C.M., DaSilva J.N., Warsh J.J., Wilson A.A., Houle S. (1999). Imaging of cAMP-specific phosphodiesterase-IV: comparison of [11C]rolipram and [11C]Ro 20-1724 in rats. Synapse.
16 Schneider H.H., Schmiechen R., Brezinski M., Seidler J. (1986). Stereospecific binding of the antidepressant rolipram to brain protein structures. Eur J Pharmacol.
17 Parker C.A., Matthews J.C., Gunn R.N., Martarello L., Cunningham V.J., Dommett D., Knibb S.T., Bender D., Jakobsen S., Brown J., Gee A.D. (2005). Behaviour of [11C]R(-)- and [11C]S(+)-rolipram in vitro and in vivo, and their use as PET radiotracers for the quantificative assay of PDE4. Synapse.
18 Fujita M., Zoghbi S.S., Crescenzo M.S., Hong J., Musachio J.L., Lu J.Q., Liow J.S., Seneca N., Tipre D.N., Cropley V.L., Imaizumi M., Gee A.D., Seidel J., Green M.V., Pike V.W., Innis R.B. (2005). Quantification of brain phosphodiesterase 4 in rat with (R)-[11C]Rolipram-PET. Neuroimage.
19 Tsukada H., Harada N., Ohba H., Nishiyama S., Kakiuchi T. (2001). Facilitation of dopaminergic neural transmission does not affect [(11)C]SCH23390 binding to the striatal D(1) dopamine receptors, but the facilitation enhances phosphodiesterase type-IV activity through D(1) receptors: PET studies in the conscious monkey brain. Synapse.
20 Tsukada H., Harada N., Nishiyama S., Ohba H., Kakiuchi T. (2000). Cholinergic neuronal modulation alters dopamine D2 receptor availability in vivo by regulating receptor affinity induced by facilitated synaptic dopamine turnover: positron emission tomography studies with microdialysis in the conscious monkey brain. J Neurosci.
21 Harada N., Nishiyama S., Ohba H., Sato K., Kakiuchi T., Tsukada H. (2002). Age differences in phosphodiesterase type-IV and its functional response to dopamine D1 receptor modulation in the living brain: a PET study in conscious monkeys. Synapse.